# Single-chain anti-epidermal growth factor receptor antibody fragment conjugated to functionalized quantum dots

Chemical name: | Single-chain anti-epidermal growth factor receptor antibody fragment conjugated to functionalized quantum dots
Abbreviated name: | ScFvEGFR-QD
Synonym:
Agent Category: | Single-chain antibody fragment (ScFv)
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Fluorescence imaging
Source of signal / contrast: | Quantum dots (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Single+chain+anti+EGFR+antibody+conjugated+to+quantum+dots)]

The epidermal growth factor receptor (EGFR) family is a group of transmembrane glycoproteins that mediate their activity through a tyrosine kinase (TK) and regulate several normal cell functions such as growth, differentiation, proliferation, and angiogenesis (1, 2). The structure of the receptor and its various ligands are discussed elsewhere (3). A mutated EGFR or its overexpression have been correlated to various malignancies and indicate a poor therapeutic outcome for the patient (4-7). Because of its established role in the initiation, development, and metastasis of many malignant tumors, EGFR was identified as an excellent target for the treatment of cancers (8). Mishani et al. and Krause and Baumann have described various labeled monoclonal antibodies (MAbs), directed toward the extracellular (EC) domain of the EGFR because of their high target specificity, and small-molecule drugs (inhibitors directed toward the intracellular TK) that are often used alone or in combination with other drugs for the diagnosis or treatment of cancer under preclinical or clinical conditions (4, 8). However, the use of MAbs for the treatment of cancer has limitations because the large size of the molecules and long blood circulation half-lives were observed to be an impediment for their distribution within a tumor. Also, due to MAb excretion primarily through the hepatic route, radioactivity from labeled MAbs that have been used to detect cancer tends to accumulate in the liver and masks the detection of any tumors in this organ (9). In addition, cancer patients treated with TK inhibitors often develop resistance to these small-molecule drugs (10). Moreover, in general, patients treated with an anti-cancer MAb or a small-molecule drug show only a modest response to the treatment (11).

In an effort to circumvent limitations observed in cancer treatment with the bulky MAbs (~160 kDa), investigators have engineered smaller (~25–30 kDa) single-chain antibody fragments (ScFv) that consist of the heavy and light variable chains of an antibody linked with a flexible peptide. The ScFv fragments are approximately five times smaller than the native MAbs, and they have been reported to have the same affinity and specificity for the target antigen as the parent MAbs (12). On the basis of the assumption that the ScFv fragments could show superior efficacy compared with the intact MAbs used for cancer therapy, investigators identified, expressed, and purified different ScFv fragments against the EGFR EC and characterized them under in vitro conditions (13, 14). Zhou et al. (14) also investigated the binding and uptake of liposomal nanoparticles (NP) bearing the ScFv fragments directed against the EGFR EC (ScFvEGFR) using tumor cells overexpressing the EGFR (for a description of the various types of NPs and their uses, click here (PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=nanoparticles))). Results obtained from that study showed that the liposomal ScFvEGFR could easily bind to the EGFR, was internalized by the tumor cells, and showed no cytotoxicity.

Yang et al. conjugated a ScFvEGFR to functionalized quantum dots (QDs), which are fluorescent NPs, to obtain ScFvEGFR-QDs and investigated their binding and internalization by EGFR-expressing cancer cells (15). Using a fluorescent imaging technique, the investigators demonstrated that ScFvEGFR-QDs specifically bound to and were internalized by EGFR-expressing cancer cells. In addition, the use of ScFvEGFR-QDs as a molecular imaging agent was demonstrated in an orthotopic human pancreatic cancer mouse xenograft model.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+QD+synthesis)]

The synthesis of ScFvEGFR-QDs was described by Yang et al. (15). Briefly, QDs with an emission at 580 nm were synthesized and coated with amphiphilic copolymers as described elsewhere (16, 17). The QDs were then conjugated through the carboxyl group on the amphiphilic copolymer surface to nickel-nitriloacetic acid (Ni-NTA) through its amino residue. The product particles, Ni-NTA-QDs, were then mixed with the ScFvEGFR containing a six-histidine tag in a 20:1 ratio in phosphate-buffered saline (PBS). The mixture was incubated at 4°C overnight, and the final ScFvEGFR-QD conjugate was purified on a Nanosep 100K OMEGA filter column. The number of ScFvEGFR linked to each QD, and the storage conditions and stability of ScFvEGFR-QDs, were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

The specificity and internalization of ScFvEGFR-QDs and non-targeted QDs were investigated using various human cancer cell lines (15). To determine specificity, the ScFvEGFR-QDs and non-targeted QDs were incubated respectively with MDA-MB-231(human breast cancer cell line that is high EGFR expressing), and MCF-7 (human breast cancer cell line with low EGFR expression) cells grown on slides for 1 h at 37°C. The cells were then washed with PBS, fixed with ice-cold acetone, and examined under a fluorescence microscope. Only cells exposed to ScFvEGFR-QDs showed a red fluorescence on the cell surface, and no signal was observed with cells exposed to the non-targeted QDs.

To investigate internalization of the ScFvEGFR-QDs, MDA-MB-231 (high EGFR expression) and MCF-7 (low EGFR expression) cells grown on slides were exposed to either ScFvEGFR-QDs or the non-targeted QDs for 2 h at 37°C (15). The cells were then washed with PBS and fixed with ice-cold acetone. The fixed cells were examined under a fluorescence confocal microscope, and a strong signal was observed inside only the MDA-MB-231 cells exposed to ScFvEGFR-QDs. A weak signal was seen with the MCF-7 cells under the same experimental conditions. No signal was obtained with cells exposed to the non-targeted QDs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+QD+rodentia)]

The biodistribution of ScFvEGFR-QDs was compared with that of the non-targeted QDs in nude mice bearing human pancreatic cancer cell line (MIA PaCa-2) xenograft tumors (15). The number of animals used for the two QD types in the study was not reported. The animals were injected through the tail vein with either ScFvEGFR-QDs or non-targeted QDs. The mice were euthanized 5 h after injection, and the tumors, along with the normal tissue, were removed to be frozen in nitrogen. The frozen sections of the various tissues were obtained and observed under either a fluorescence or a confocal microscope. Compared with the non-targeted QDs, only the ScFvEGFR-QDs were observed in the tumor tissue with fluorescence microscopy. Observation of the tumor tissue under the confocal microscope showed that the ScFvEGFR-QDs were internalized by the tissue. An examination of the normal tissue with fluorescence microscopy revealed that the non-targeted QDs were present primarily in the liver, followed by the spleen, and at low and very low levels in the lungs and kidneys, respectively. Low levels of ScFvEGFR-QDs were detected in the liver and spleen, and very low levels were detected in the lungs and kidneys. From these observations, the investigators concluded that ScFvEGFR-QDs could possibly be used as in vivo tumor imaging agents.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+QD+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ScFvEGFR+QD+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

### NIH Support

Some of the studies reported in this chapter were funded by NIH Grants P50-CA58207 and CA119338-01.

### References

1 Huang Z., Brdlik C., Jin P., Shepard H.M. (2009). A pan-HER approach for cancer therapy: background, current status and future development. Expert Opin Biol Ther.
2 Diagaradjane P., Orenstein-Cardona J.M., Colon-Casasnovas N.E., Deorukhkar A., Shentu S., Kuno N., Schwartz D.L., Gelovani J.G., Krishnan S. (2008). Imaging epidermal growth factor receptor expression in vivo: pharmacokinetic and biodistribution characterization of a bioconjugated quantum dot nanoprobe. Clin Cancer Res.
3 Schneider M.R., Wolf E. (2009). The epidermal growth factor receptor ligands at a glance. J Cell Physiol.
4 Mishani E., Abourbeh G., Eiblmaier M., Anderson C.J. (2008). Imaging of EGFR and EGFR tyrosine kinase overexpression in tumors by nuclear medicine modalities. Curr Pharm Des.
5 Lievre A., Bachet J.B., Le Corre D., Boige V., Landi B., Emile J.F., Cote J.F., Tomasic G., Penna C., Ducreux M., Rougier P., Penault-Llorca F., Laurent-Puig P. (2006). KRAS mutation status is predictive of response to cetuximab therapy in colorectal cancer. Cancer Res.
6 Ke S., Wen X., Gurfinkel M., Charnsangavej C., Wallace S., Sevick-Muraca E.M., Li C. (2003). Near-infrared optical imaging of epidermal growth factor receptor in breast cancer xenografts. Cancer Res.
7 Charpidou A., Blatza D., Anagnostou E., Syrigos K.N. (2008). Review. EGFR mutations in non-small cell lung cancer--clinical implications. In Vivo.
8 Krause M., Baumann M. (2008). Clinical biomarkers of kinase activity: examples from EGFR inhibition trials. Cancer Metastasis Rev.
9 Pantaleo, M.A., M. Nannini, A. Maleddu, S. Fanti, C. Nanni, S. Boschi, F. Lodi, G. Nicoletti, L. Landuzzi, P.L. Lollini, and G. Biasco, Experimental results and related clinical implications of PET detection of epidermal growth factor receptor (EGFr) in cancer. Ann Oncol, 2008
10 Engelman J.A., Settleman J. (2008). Acquired resistance to tyrosine kinase inhibitors during cancer therapy. Curr Opin Genet Dev.
11 Vogel C.L., Cobleigh M.A., Tripathy D., Gutheil J.C., Harris L.N., Fehrenbacher L., Slamon D.J., Murphy M., Novotny W.F., Burchmore M., Shak S., Stewart S.J., Press M. (2002). Efficacy and safety of trastuzumab as a single agent in first-line treatment of HER2-overexpressing metastatic breast cancer. J Clin Oncol.
12 Honegger, A., Engineering antibodies for stability and efficient folding. Handb Exp Pharmacol, 2008(181): p. 47-68.
13 Horak E., Heitner T., Robinson M.K., Simmons H.H., Garrison J., Russeva M., Furmanova P., Lou J., Zhou Y., Yuan Q.A., Weiner L.M., Adams G.P., Marks J.D. (2005). Isolation of scFvs to in vitro produced extracellular domains of EGFR family members. Cancer Biother Radiopharm.
14 Zhou Y., Drummond D.C., Zou H., Hayes M.E., Adams G.P., Kirpotin D.B., Marks J.D. (2007). Impact of single-chain Fv antibody fragment affinity on nanoparticle targeting of epidermal growth factor receptor-expressing tumor cells. J Mol Biol.
15 Yang L., Mao H., Wang Y.A., Cao Z., Peng X., Wang X., Duan H., Ni C., Yuan Q., Adams G., Smith M.Q., Wood W.C., Gao X., Nie S. (2008). Single Chain Epidermal Growth Factor Receptor Antibody Conjugated Nanoparticles for in vivo Tumor Targeting and Imaging. Small.
16 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
17 Smith, A.M., H. Duan, M.N. Rhyner, G. Ruan, and S. Nie, A systematic examination of surface coatings on the optical and chemical
(2006). properties of semiconductor quantum dots. Physical Chemistry Chemical Physics.